# ^111^In-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-{Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_}_2_

Chemical name: | ^111^In-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-{Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_}_2_
Abbreviated name: | ^111^In-DOTA-E-{E-[c(RGDfK)]_2_}_2_
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | SPECT, gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). Extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) contain a tripeptide sequence consisting of Arg-Gly-Asp (RGD), which binds to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Dijkgraaf et al. (13) reported the development of ^111^In-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-{Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_}_2_ (^111^In-DOTA-E-{E-[c(RGDfK)]_2_}_2_) for imaging α_v_β_3_ receptors in nude mice bearing ovarian carcinoma tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+RGD+synthesis)]

Dijkgraaf et al. (13) prepared the synthesis of ^111^In-DOTA-E-{E-[c(RGDfK)]_2_}_2_ by reacting 4.8 nmol DOTA-E-{E-[c(RGDfK)]_2_}_2_ with 13 MBq (0.35 mCi) ^111^InCl_3_ in ammonium acetate buffer at 100°C for 15 min. Radiochemical purity was >93% as determined by high-performance liquid chromatography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+RGD+in+vitro)]

Dijkgraaf et al. (13) performed in vitro solid-phase binding assays of ^111^In-DOTA-E-[c(RGDfK)]_2_ with human α_v_β_3_ integrin. DOTA-E-c(RGDfK) had an IC_50_ value of 120 nM. DOTA-E-[c(RGDfK)]_2_ had an IC_50_ value of 69.9 nM. DOTA-E-{E-[c(RGDfK)]_2_}_2_ had an IC_50_ value of 19.6 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+RGD+rodentia)]

Dijkgraaf et al. (13) performed biodistribution studies of ^111^In-DOTA-E-{E-[c(RGDfK)]_2_}_2_ in nude mice bearing SK-RC-52 human renal cell carcinoma tumors. The tumor uptake of the tetramer (7.40 ± 1.12% injected dose (ID)/g) was significantly higher than that of the monomer (2.30 ± 0.34% ID/g), and the dimer (5.17 ± 1.22% ID/g) at 8 h after injection. The tumor uptake was significantly higher for the tetramer (6.82 ± 1.41% ID/g) than for the dimer (4.22 ± 0.96% ID/g) and the monomer (1.90 ± 0.29% ID/g) at 24 h. The intestine, kidney, liver, and spleen had high levels of radioactivity. Co-injection of 50 ug E-[c(RGDfK)]_2_ with 0.5 μg ^111^In-DOTA-E-{E-[c(RGDfK)]_2_}_2_ reduced tumor uptake by >85%. The accumulation was also markedly reduced in the intestine, liver, lung, and spleen (this may be partly mediated by α_v_β_3_ integrin in these tissues) but not in the kidney.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+RGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+RGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+RGD+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Dijkgraaf I., Kruijtzer J.A., Liu S., Soede A.C., Oyen W.J., Corstens F.H., Liskamp R.M., Boerman O.C. (2007). Improved targeting of the alpha(v)beta (3) integrin by multimerisation of RGD peptides. Eur J Nucl Med Mol Imaging.
14 Janssen M.L., Oyen W.J., Dijkgraaf I., Massuger L.F., Frielink C., Edwards D.S., Rajopadhye M., Boonstra H., Corstens F.H., Boerman O.C. (2002). Tumor targeting with radiolabeled alpha(v)beta(3) integrin binding peptides in a nude mouse model. Cancer Res.